# 1(trans-[^123^I]Iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]piperidine

Chemical name: | 1(trans-[^123^I]Iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]piperidine
Abbreviated name: | [^123^I]TPCNE
Synonym: | [^123^I]1-(4-Cyanobenzyl)-4-[[(trans-iodopropen-2-yl)oxy]methyl]piperidine
Agent Category: | Compound
Target: | Sigma (σ) receptors
Target Category: | Receptor binding
Method of detection: | Single photon emission computed tomography (SPECT)
Source of signal/contrast: | ^123^I
Activation: | No
Studies: | - In vitro; - Rodents; - Humans | Click on the above structure for additional information in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29)]

1(trans-[^123^I]Iodopropen-2-yl)-4-[(4-cyanophenoxy)methyl]piperidine ([^123^I]TPCNE) is a radioligand developed for single photon emission computed tomography (SPECT) imaging of the sigma (σ) receptors (1, 2). [^123^I]TPCNE is a highly selective σ_1_ receptor radioligand labeled with ^123^I, a gamma emitter with a physical half-life (t_½_) of 13.2 h.

The σ receptors are functional, membrane-bound, G-protein–coupled receptors that are distributed in the central nervous system (CNS) and peripheral organs (3). The CNS σ receptors are unique binding sites related to higher brain functions (4). They are distinct from opiate and phencyclidine binding sites. There are at least two subtypes of σ receptors: σ_1_ and σ_2_ receptors. The precise mechanism of the functional response of these receptors is not entirely known. These receptors appear to be involved in numerous pharmacological and physiological functions, and they also modulate a number of central neurotransmitter systems, including noradrenergic, glutamatergic, and dopaminergic systems. Phencyclidine and derivatives, cocaine and derivatives, some neuroleptics, atypical antipsychotic agents, and other chemically unrelated compounds are able to bind to the σ receptor sites. Studies have shown that these receptors may play a role in the pathogenesis of psychiatric disorders (5, 6). These receptors are also expressed on a number of human and murine tumors (7).

The σ_1_ receptor subtypes have a molecular mass of ≈25 kDa, and through the process of cloning they have shown a 30% sequence homology with the yeast C89-C7 sterol isomerase (3, 8, 9). The σ_2_ receptor subtypes have a molecular weight of ≈21.5 kDa, and they have not been cloned. The σ_1_ receptors are thought to be involved in certain neuropsychiatric disorders, and the σ_2_ receptors are implicated in malignant neoplastic diseases. Because of these effects, σ receptor ligands may be useful for detection and treatment in neurology and oncology. A number of ligands for these receptors have been labeled with radionuclides for SPECT and positron emission tomography (PET) imaging to map their in vivo brain distribution and expression on tumors (10). Watanabe et al. (11) showed that a tritiated compound, [^3^H]DuP 734, had high affinity and selectivity for σ receptors and good brain uptake in mice. However, this compound also had high affinity for serotonin (5HT_2_) receptors in vitro. Gilligan et al. (12) studied the structure-activity relationships of a series of more selective analogs that included 1-benzyl-4-[[(cyclopropylmethyl)oxy]methyl]piperidine. The study showed that a wide variety of lipophilic groups could be attached to the ether linkage without a significant effect on the σ receptor affinity. On the basis of this finding, Waterhouse et al. (2) proposed that the cyclopropylmethyl group could be replaced by a radioiodinated iodopropenyl group to provide a radioligand for σ receptor imaging. [^123^I]TPCNE was designed and synthesized from this concept with an additional cyano group added to the aromatic ring to help offset the increased lipophilicity induced by the radioactive iodine atom.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20synthesis)]

Waterhouse et al. (2) described the synthesis of a vinyl organostannane precursor for [^123^I]TPCNE radiolabeling from 4-hydroxymethylpiperidine. The radioligand was then synthesized by electrophilic radioiododestannylation of the tributyltin precursor at acidic pH using chloramine-T dehydrate as the oxidant. Briefly, 4-hydroxymethylpiperidine was alkylated by reacting with 4-cyanobenzyl bromide in dichloromethane and potassium carbonate to give 1-(4-cyanobenzyl)-4-hydroxymethylpiperidine (58% yield). This sodium alkoxide salt was reacted with propargyl bromide in tetrahydrofuran and sodium hydride to produce a propargyl ether, 1-(4-cyanobenzyl)-4-[[(propargyl)oxy]methyl]piperidine (78% yield). This was then reacted with tri-n-butyltin hydride in the presence of a radical initiator to form the trans-vinyl stannane precursor 1-(4-cyanobenzyl)-4-[[(trans-tri-n-butyltinpropen-2-yl)-oxy]methyl]piperidine (71% yield). In the radiolabeling procedure, chloramine-T dissolved in methanol and water was added to sodium [^123^I]iodide ([^123^I]NaI) in sodium hydroxide solution acidified by acetic acid. The precursor was added immediately, and the radiolabeling was allowed to proceed for 1 min before quenching with sodium metasulfite. The radiolabeled ligand was purified by high-performance liquid chromatography (HPLC). The radiochemical yield was 68.4 ± 5.1% (n = 5) at the end of synthesis, and the radiochemical purity was >99%. The specific activity was determined to be >77,000 MBq/μmol (2,100 mCi/μmol).

Stone et al. (1) reported that the use of hydrogen peroxide (H_2_O_2_) as the oxidant to reduce the amount of precursor from 1 mg to 50 μg improved radiolabeling in human studies. In this method, [^123^I]NaI was first acidified by hydrochloric acid. The tributyltin precursor dissolved in ethanol and H_2_O_2_ were added to the [^123^I]NaI solution. The resulting radiolabeled ligand was purified by HPLC. To use this radioligand in humans, [^123^I]TPCNE was reformulated by extraction with a C18 cartridge and sterilization by filtration. The product was analyzed before injection into humans. The final radiochemical yield was 50–55%. The specific activity was >58 GBq/μmol (1.57 Ci/μmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20in%20vitro)]

Waterhouse et al. (2) determined the lipophilicity of TPCNE by the HPLC method using standards of known log P values. The log P_7.5_ value of TPCNE was 3.24. In vitro receptor competitive binding assays were performed by the NIMH/NovaScreen Discovery & Development Program to determine the affinity and specificity of [^123^I]TPCNE. The inhibition constant (K_i_) values of TPCNE were 0.38 nM and 21.3 nM for σ_1_ and σ_2_, respectively. The K_i_ σ_1_/σ_2_ ratio was 0.02. The affinity of TPCNE to 5HT_2_ receptors was negligible (K_i_ >10,000 nM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20rodentia)]

Waterhouse et al. (2) examined the biodistribution of [^123^I]TPCNE from 10 min to 240 min in rats (n = 3). There was a prolonged retention of radioactivity in the brain, heart, lungs, and other organs known to contain σ receptors. The radioactivity levels in the thyroid (unblocked) were relatively low, from 0.03 ± 0.00% injected dose/g (% ID/g) at 10 min after injection to 0.26 ± 0.02% ID/g at 240 min after injection. This indicated a slow in vivo deiodination of [^123^I]TPCNE. The radioactivity levels (% ID/g) in major organs at 20 min were 14.11 ± 1.98 (lungs), 1.57 ± 0.20 (heart), 1.40 ± 0.21 (kidney), 0.06 ± 0.01 (blood), and 0.10 ± 0.01 (liver). The radioactivity levels (% ID/g) in the brain at 20 min were 1.11 ± 0.14 (whole brain), 0.09 ± 0.02 (posterior cortex), 0.85 ± 0.16 (frontal cortex), 0.56 ± 0.12 (striatum), and 0.57 ± 0.10 (cerebellum). These levels increased to 1.49 ± 0.14 (whole brain), 1.14 ± 0.05 (posterior cortex), 1.02 ± 0.11 (frontal cortex), 0.74 ± 0.10 (striatum), and 0.75 ± 0.11 (cerebellum) at 240 min.

Specific binding studies were performed by giving unlabeled TPCNE, DuP 734 (σ, 5HT_2_), and haloperidol (dopamine D_2_, σ) at a dose of 1 mg/kg at 5 min before the radioligand injection (10 μCi/rat) (2). The study reported that a significant reduction of radioactivity (P < 0.01) at 30 min after injection was observed in all brain regions and peripheral organs known to contain σ receptors. In the brain regions, the radioactivity levels were reduced by 50–80% (P < 0.001, extrapolation from Figure 4), with the biggest blocking effect by TPCNE, and the effect of DuP 734 was greater than that of haloperidol.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28%5B123I%5DTPCNE%20OR%20%28halogenated%204-%28Phenoxymethyl%29piperidines%29%29%20AND%20human)]

Human studies of [^123^I]TPCNE were performed in 7 healthy volunteers (1). Each subject received a single bolus i.v. dose of ≈180 MBq (5 mCi) of [^123^I]TPCNE and scanned from the time of injection until 3–3.5 h after injection. Whole-body imaging revealed that the radioactivity distribution pattern was different from rats. In humans, the liver and brain showed the greatest radioactivity level. Radioactivity uptake was rapid in the brain with a widespread distribution. The brain uptake kinetics appeared to be best described by an irreversible model. The total brain radioactivity reached ≈8.7% ID in 30 min and remained almost constant for 3–3.5 h. The posterior cingulate had the highest radioactivity level with an irreversible model effective uptake rate constant (K) of ≈0.33 (estimated from Figure 7), which was proportional to regional binding. The cerebellum and thalamus had a similar K value of ≈0.30. The striatum and white matter had K values of ≈0.26 and ≈0.13, respectively. When subjects received an oral dose of 2.5 mg of haloperidol ≈1 h before the study, there was a clear washout in all brain regions. Displaceable [^123^I]TPCNE binding was estimated to be 73% in the thalamus, 58% in the posterior cingulate, 42% in the cerebellum, and 20% in the white matter. The authors suggested that the binding distribution and kinetics of [^123^I]TPCNE were similar to those of two other σ PET ligands, [^18^F]FPS and [^11^C]SA4503.

Arterial sampling was performed during the scans and the in vivo metabolism of [^123^I]TPCNE was determined by HPLC analysis of the plasma samples (1). The radioactivity in the blood peaked at ≈45 s, and then a rapid clearance was observed. At 30 min, <1% of the peak radioactivity level was found. The metabolism study showed that ≈80% of [^123^I]TPCNE remained unchanged at 67 min after injection. Only one labeled highly polar metabolite appeared at 45 min.

## NIH Support

NIMH-2003.

## References

1 Stone J.M., Arstad E., Erlandsson K., Waterhouse R.N., Ell P.J., Pilowsky L.S. (2006). [123I]TPCNE--a novel SPECT tracer for the sigma-1 receptor: first human studies and in vivo haloperidol challenge. Synapse.
2 Waterhouse R.N., Mardon K., O'Brien J.C. (1997). Synthesis and preliminary evaluation of [123I]1-(4-cyanobenzyl)-4-[[(trans-iodopropen-2-yl)oxy]meth yl]piperidine: a novel high affinity sigma receptor radioligand for SPECT. Nucl Med Biol.
3 Lever J.R., Gustafson J.L., Xu R., Allmon R.L., Lever S.Z. (2006). Sigma1 and sigma2 receptor binding affinity and selectivity of SA4503 and fluoroethyl SA4503. Synapse.
4 Skuza G., Wedzony K. (2004). Behavioral pharmacology of sigma-ligands. Pharmacopsychiatry.
5 Skuza G. (2003). Potential antidepressant activity of sigma ligands. Pol J Pharmacol.
6 Ishiguro H., Ohtsuki T., Toru M., Itokawa M., Aoki J., Shibuya H., Kurumaji A., Okubo Y., Iwawaki A., Ota K., Shimizu H., Hamaguchi H., Arinami T. (1998). Association between polymorphisms in the type 1 sigma receptor gene and schizophrenia. Neurosci Lett.
7 Vilner B.J., John C.S., Bowen W.D. (1995). Sigma-1 and sigma-2 receptors are expressed in a wide variety of human and rodent tumor cell lines. Cancer Res.
8 Mach R.H., Gage H.D., Buchheimer N., Huang Y., Kuhner R., Wu L., Morton T.E., Ehrenkaufer R.L. (2005). N-[18F]4'-fluorobenzylpiperidin-4yl-(2-fluorophenyl) acetamide ([18F]FBFPA): a potential fluorine-18 labeled PET radiotracer for imaging sigma-1 receptors in the CNS. Synapse.
9 Hanner M., Moebius F.F., Flandorfer A., Knaus H.G., Striessnig J., Kempner E., Glossmann H. (1996). Purification, molecular cloning, and expression of the mammalian sigma1-binding site. Proc Natl Acad Sci U S A.
10. Mahmood, A. and A.G. Jones, Techneitum Radiopharmaceuticals, in Handbooks of Radiopharmaceuticals, M.J. Welch and C.S. Redvanley, Editors. 2003, John Wiley & Sons, Ltd.: West Sussex. p. 323-349.
11 Watanabe M., Rominger D., Hurt S.D., De Souza E.B., Tam S.W. (1993). [3H]1-(cyclopropylmethyl)-4-(2-(4-fluorophenyl)-2-oxoethyl) piperidine HBr (DuP 734). A selective ligand for sigma receptors in mouse brain in vivo. J Pharmacol Exp Ther.
12 Gilligan P.J., Cain G.A., Christos T.E., Cook L., Drummond S., Johnson A.L., Kergaye A.A., McElroy J.F., Rohrbach K.W., Schmidt W.K., et al. (1992). Novel piperidine sigma receptor ligands as potential antipsychotic drugs. J Med Chem.